# (E)-4-(2-(6-(2-(2-(2-([^18^F]-fluoroethoxy)ethoxy)ethoxy)pyridin-3-yl)vinyl)-N-methylbenzenamine

Chemical name: | (E)-4-(2-(6-(2-(2-(2-([^18^F]-fluoroethoxy)ethoxy)ethoxy)pyridin-3-yl)vinyl)-N-methyl benzenamine
Abbreviated name: | [^18^F]AV-45
Synonym: | [^18^F]Florbetapir
Agent category: | Compound
Target: | Amyloid-beta peptide
Target category: | Acceptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-45)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions overtime (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of amyloid-beta peptides consisting of 40 to 42 amino acids) and intracellular neurofibrillary tangles (filaments of microtubule-binding hyper-phosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). β-amyloid peptides and tau protein are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various β-amyloid imaging agents have been developed for magnetic resonance imaging (MRI), single photon emission computed tomography (SPECT), and positron emission tomography (PET) (8-13). The binding of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human post-mortem brain tissue and in transgenic mice. Out of these analogues, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) was studied in humans, showing more binding in the brains of patients with AD than in those of healthy people (14). However, [^18^F]FDDNP showed low signal-to-noise ratios for PET imaging, because it is highly lipophilic. N-methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a β-amyloid binding compound based on a series of neutral thioflavin-T derivatives (15), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for the senile plaques in the brain (16). Zhang et al. (17) reported the development of a series of fluorinated polyethylene glycol (PEG) units (n = 2-5) for PET imaging of β-amyloid plaques in the brain. Two of them, [^18^F]{4-[2-(4-{2-(2[2-(2-Fluoro-ethoxy)-ethoxyl]-ethoxy}-phenyl)-vinyl]-phenyl}-methyl-amine ([^18^F]BAY94-9172, [^18^F]AV-1) (18) and (E)-4-(2-(6-(2-(2-(2-([^18^F]-fluoroethoxy)ethoxy)ethoxy)pyridin-3-yl)vinyl)-N-methyl benzenamine ([^18^F]AV-45) (19), are being evaluated in clinical trials.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid)
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid))
- Drug information in FDA (Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-45%20and%20synthesis)]

[^18^F]AV-45 was readily synthesized by standard ^18^F-fluorination of N-BOC-protected O-tosylated derivative with ([^18^F]KF/Kryptofix 2.2.2, 120°C for 10 min), followed by hydrolysis (HCl, 120°C for 5 min) (19). The radiochemical yield was 10-30% with the specific activity of 37-185 GBq/mmol (1-5 Ci/mmol) at the end of synthesis. Radiochemical purity was >99% as determined with high-performance liquid chromatography (HPLC). Total synthesis time was not reported.

Yao et al. (20) reported that [^18^F]AV-45 was prepared in 105 min using a tosylate precursor with Sumitomo modules for radiosynthesis under GMP-compliant conditions. The overall yield was 25.4 ± 7.7% with a HPLC purity of 95.3 ± 2.2% (n = 19). The specific activity of [^18^F]AV-45 was 470 ± 135 GBq/µmol (12.7 ± 3.6 Ci/µmol, n = 19).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-45%20and%20in%20vitro)]

[^18^F]AV-45 has the binding affinity (K_d_) value of 3.72 ± 0.3 nM for aggregated β-amyloid fibrils (postmortem AD brain homogenates, n = 4) and the receptor density (B_max_) value of 8.81 ± 1.64 pmol/mg protein (19). The K_i_ values for AV-45, PIB, and BAY94-9172 in competition with [^18^F]AV-45 were found to be 2.87 ± 0.17, 0.87 ± 0.18, and 2.22 ± 0.54 nM, respectively. [^18^F]AV-45 was bound to the cortex of postmortem AD brain slices but not to control brain slices as visualized by autoradiography studies.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-45%20and%20rodentia)]

[^18^F]AV-45 (0.37 MBq, 10 μCi) was injected intravenously into normal mice (n = 3/group) to study its accumulation into the brain and other organs/tissues at 2, 60, 120 and 180 min after injection (19). [^18^F]AV-45 showed an initial rapid penetration into the brain with 6.23% injected dose (ID)/g at 2 min, with a quick washout (1.84% ID/g at 60 min) in female mice and 7.33% ID/g at 2 min and 1.88% ID/g at 60 min in male mice. The organs with the highest accumulation was the liver (11.07% ID/g) and intestine (12.46% ID/g), followed by the kidney (5.94% ID/g), stomach (4.39% ID/g), and lung (2.58% ID/g) at 60 min after injection. The radioactivity levels were 2.37% and 3.66% in the blood and bone, respectively. The bone radioactivity increased to 7.83% ID/g at 180 min. The rate of defluorination indicated by the bone uptake seems high. There was about 30% intact [^18^F]AV-45 in the plasma at 30 min after injection with two major metabolites, the N-demethylated and N-acetylated derivatives of [^18^F]AV-45. Both metabolites did not show any specific binding to β-amyloid fibrils in vitro. Ex-vivo autoradiography studies of the brain after injection of [^18^F]AV-45 in the transgenic Tg2576 mice overexpressing β-amyloid plaques were performed. The brain showed a distinctive labeling of β-amyloid plaques and co-staining with thioflavin-S. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-45%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-45%20and%20primate%20not%20human)]

PET imaging was performed in the brain of one healthy young female rhesus monkey after injection of 174 MBq (4.7 mCi) [^18^F]AV-45 (19). The radioactivity (4.4% ID) peaked at the cortex at 7 min after injection with quick washout to about the background level of the brain white matter at 20 min.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-45%20and%20humans)]

Wong et al. (21) used dynamic PET imaging with [^18^F]AV-45 to study 16 patients with AD and 16 healthy elderly control patients. [^18^F]AV-45 binding was quantified by use of the standardized uptake value ratio (SUVR), which was calculated for the neocortex, with the cerebellum as reference region. Widespread neocortical binding was observed in all AD patients with a SUVR plateau at 50-60 min after injection with ~370 MBq (10 mCi) [^18^F]AV-45. A higher neocortical SUVR was observed in AD patients (1.67 ± 0.18) than in healthy controls (1.25 ± 0.18; P < 0.005) at 50-60 min. The effective dose was estimated to be 0.013 mSv/MBq (48.1 mrem/mCi). The organs with the greatest exposure were the gallbladder, liver, intestines, and urinary bladder. In a study of three patients with AD and three healthy elderly control patients, Lin et al. (22) reported also a higher SUVR in AD patients (1.51 ± 0.30) than in healthy controls (1.17 ± 0.11) at 50 min after injection with 382 MBq (10.3 mCi) [^18^F]AV-45.

## NIH Support

ROI-AG022559, R43AG032206, K24DA000412, MH078175, AA012839

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
4 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
5 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
6 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
10 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
11 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
12 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
13 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
16 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
17 Zhang W., Oya S., Kung M.P., Hou C., Maier D.L., Kung H.F. (2005). F-18 Polyethyleneglycol stilbenes as PET imaging agents targeting Abeta aggregates in the brain. Nucl Med Biol.
18 O'Keefe G.J., Saunder T.H., Ng S., Ackerman U., Tochon-Danguy H.J., Chan J.G., Gong S., Dyrks T., Lindemann S., Holl G., Dinkelborg L., Villemagne V., Rowe C.C. (2009). Radiation Dosimetry of {beta}-Amyloid Tracers 11C-PiB and 18F-BAY94-9172. J Nucl Med.
19 Choi S.R., Golding G., Zhuang Z., Zhang W., Lim N., Hefti F., Benedum T.E., Kilbourn M.R., Skovronsky D., Kung H.F. (2009). Preclinical properties of 18F-AV-45: a PET agent for Abeta plaques in the brain. J Nucl Med.
20 Yao C.H., Lin K.J., Weng C.C., Hsiao I.T., Ting Y.S., Yen T.C., Jan T.R., Skovronsky D., Kung M.P., Wey S.P. (2010). GMP-compliant automated synthesis of [(18)F]AV-45 (Florbetapir F 18) for imaging beta-amyloid plaques in human brain. Appl Radiat Isot.
21 Wong D.F., Rosenberg P.B., Zhou Y., Kumar A., Raymont V., Ravert H.T., Dannals R.F., Nandi A., Brasic J.R., Ye W., Hilton J., Lyketsos C., Kung H.F., Joshi A.D., Skovronsky D.M., Pontecorvo M.J. (2010). In vivo imaging of amyloid deposition in Alzheimer disease using the radioligand 18F-AV-45 (florbetapir [corrected] F 18). J Nucl Med.
22 Lin K.J., Hsu W.C., Hsiao I.T., Wey S.P., Jin L.W., Skovronsky D., Wai Y.Y., Chang H.P., Lo C.W., Yao C.H., Yen T.C., Kung M.P. (2010). Whole-body biodistribution and brain PET imaging with [18F]AV-45, a novel amyloid imaging agent--a pilot study. Nucl Med Biol.